# Hyperpolarized ^13^C-labeled bicarbonate (H^13^CO_3_^-^) for in vivo pH measurement with ^13^C magnetic resonance spectroscopy

Chemical name: | Hyperpolarized ^13^C-labeled bicarbonate (H^13^CO_3_^-^) for in vivo pH measurement with ^13^C magnetic resonance spectroscopy
Abbreviated name: | Hyperpolarized H^13^CO_3_^-^
Synonym: | ^13^C-bicarbonate, ^13^CO_2_
Agent Category: | Compounds
Target: | Carbonic anhydrase (tissue pH)
Target Category: | Enzymes
Method of detection: | Magnetic resonance imaging (MRI)/magnetic resonance spectroscopy (MRS)
Source of signal / contrast: | Hyperpolarized ^13^C
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Magnetic+resonance+spectroscopy)]

Magnetic resonance spectroscopy (MRS) is a technique that allows the non-invasive detection of multiple small metabolites within cells or extracellular spaces in vivo (1-4). Although MRS is theoretically applicable to any nucleus possessing spin, the more frequently investigated applications are in proton (^1^H) and carbon-13 (^13^C) (5-7). ^13^C MRS is superior to ^1^H MRS in many respects (3, 7-9). ^13^C MRS can provide specific information about the identity and structure of biologically important compounds. The chemical shift range for carbon (~250 ppm) is much larger than that for proton (~15 ppm), allowing for improved resolution of metabolites. However, ^13^C MRS is limited by the low natural abundance of ^13^C (1.1%) and its very low nuclear spin polarization (2.5 × 10^-6^ polarization at 3 T and 37ºC) (2, 3). Several techniques have been used to overcome these limitations, including dynamic nuclear polarization (DNP), which introduces one or more ^13^C molecules into a metabolic substrate (2, 3, 9). Because the T_1_ relaxation time of ^13^C in small molecules is much longer than that of ^1^H (0.1–2.0 s in a magnetic field of 0.1–3.0 T), hyperpolarized ^13^C-labeled tracers can be generated outside the subject and the magnetic resonance scanner (7). Nearly 100% nuclear polarization for ^1^H and 50% for ^13^C can be achieved in various organic molecules when DNP is performed in a strong magnetic field and at cryogenic temperatures. Replacing the ^12^C isotope (98.9% natural abundance) with the ^13^C isotope at a specific carbon or carbons in a metabolic substrate does not affect the substrate’s biochemistry. Hyperpolarized ^13^C-labeled substrates can provide >10,000-fold enhancement of the ^13^C MRS signals from the substrate and its subsequent metabolic products, allowing the assessment of changes in metabolic fluxes in vivo and the imaging of blood vessels and tissue perfusion without background signal from surrounding tissues (1, 3, 4, 10-14).

^13^C MRS with DNP technique has also been investigated for measuring tissue pH in vivo (4, 15). HCO_3_^-^ is the primary extracellular buffer, and it resists changes in pH through interconversion with CO_2_ in the reaction catalyzed by carbonic anhydrase. In principal, tissue pH can be determined from ^13^C MRS measurements of endogenous H^13^CO_3_^-^ and ^13^CO_2_ because their concentration ratio can be used to calculate pH from the Henderson-Hasselbalch equation with an acid dissociation constant (pKa) of 6.17 in vivo. On the basis of this principal, Schroeder et al. measured the pH in diseased and healthy cardiac myocytes with simultaneous detection of hyperpolarized [1-^13^C]pyruvate-derived H^13^CO_3_^-^ and ^13^CO_2_ (15). Their results suggest that hyperpolarized [1-^13^C]pyruvate with MRS detection of its derived H^13^CO_3_^-^ and ^13^CO_2_ can be used to measure the intracellular pH (pH_i_) of cardiomyocytes in vivo. Similarly, Gallagher et al. generated a non-toxic, pH-probe, hyperpolarized H^13^CO_3_^-^ and exploited the pH in tumors with measurement of the H^13^CO_3_^-^ and ^13^CO_2_ concentration ratio after administration of hyperpolarized H^13^CO_3_^-^ (4).

The tumor microenvironment is characterized by low extracellular pH (pH_e_) and neutral-to-alkaline pH_i_ (16, 17). The average pH_e_ could be as low as 6.0. A pH gradient (pH_i_ > pH_e_) exists across the cell membrane in tumors. This gradient is contrary to that found in normal tissues, in which pH_i_ (7.2–7.4) is lower than pH_e_. In addition, diffusion of the H^+^ ions along concentration gradients from tumors into adjacent normal tissues creates a peritumoral acid gradient. Accurate measurement of the pH in tissues is of diagnostic and therapeutic value. Imaging with small-molecule agents has been tested for measuring tumor pH. However, agents based on ^1^H, ^31^P, or ^19^F MRS are limited by the inherent low sensitivity of spectroscopy and small pH-dependent chemical shift of these agents (18, 19). The approach with gadolinium (Gd^3+^) chelate relaxation agents, which show a pH-dependent hydrogen exchange to the Gd^3+^-bound water, requires an accurate determination of the agent concentration, which in practice is difficult to achieve in vivo (20). Although positron emission tomography and optical imaging are sensitive, they appear have difficulty obtaining a pH map at high resolution (21-23). Furthermore, most of the published probes predominantly measure the pH within cells, which is more resistant to pH changes than the extracellular space. The data obtained by Gallagher et al. from hyperpolarized H^13^CO_3_^-^ indicated that hyperpolarized H^13^CO_3_^-^ provided a means to measure the pH_e_ rather than the pH_i_ (4). Given the range of pathological conditions in which the acid–base balance is altered, this technique may prove to be of diagnostic value not only in oncology but also in the imaging of ischemia and inflammation (4).

### Related Resource Links:

- Chapters of ^13^C MRS in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=13C%2C+MRI+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Carbonic anhydrase in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=136850)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=hyperpolarized+13C-labelled+bicarbonate)]

Gallagher et al. described the generation of hyperpolarized H^13^CO_3_^-^ in detail (4). Briefly, CsH^13^CO_3_ was first prepared by slowly adding ^13^CO_2_ to CsOH hydrate. Up to 98% of the bicarbonate was labeled with ^13^C at this step. ^13^C-Labeled CsH^13^CO_3_ was then dissolved in water and glycerol. After addition of free radical (OX063) and Gd^3+^ chelate, the solution was polarized in a polarizer under a 93.982 GHz and 100-mW microwave source for 2 h. The frozen sample was dissolved in phosphate buffer (pH 7.5) containing diaminoethane tetraacetic acid heated to 180°C and pressurized to 10 bar. Cs was rapidly removed with an ion-exchange column to generate the pure hyperpolarized H^13^CO_3_^-^. The final concentration of H^13^CO_3_^-^ was ~100 mmol at 37°C. The polarized H^13^CO_3_^-^ was 16% in the solution state, which represents a 20,000-fold increase above thermal equilibrium (at 9.4 T and 37°C).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=hyperpolarized+13C-labelled+bicarbonate)]

Gallagher et al. first tested the feasibility to measure the pH in phosphate buffers in vitro with hyperpolarized H^13^CO_3_^-^ (4). The pH in each voxel was calculated from the relative concentrations of H^13^CO_3_^-^ and ^13^CO_2_ with the Henderson-Hasselbalch equation. In the presence of carbonic anhydrase in buffers, the estimated pH was closely correlated with that measured using a pH meter (average pH difference ± SD, 0.07 ± 0.03; n = 4) but was slightly overestimated in the absence of the enzyme (0.32 ± 0.13; n = 6) (P = 0.01). This close correlation reflects the rapid establishment of chemical equilibrium and equilibration of polarization between H^13^CO_3_^-^ and ^13^CO_2_ catalyzed by carbonic anhydrase.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=hyperpolarized+13C-labelled+bicarbonate)]

Gallagher et al. performed ^13^C spectra and spectroscopic imaging (at 9.4 T) in mice bearing murine lymphoma tumors (4). One group of mice was pretreated with ammonium chloride to decrease the tissue pH, and another group of mice was pretreated with sodium bicarbonate solution to increase the tissue pH. ^31^P spectra were also acquired after the intraperitoneal administration of 3-aminopropylphosphonate (3-APP) for comparative study. Spectra of H^13^CO_3_^-^ and ^13^CO_2_ from tumor slices (5 mm thick) gave a calculated pH of 6.71 ± 0.14 (n = 12) compared with a non–slice-selective pH, which included a weighted mean of the tumor pH and that of surrounding tissue, of 7.09 ± 0.10 (n = 8) (P < 0.01). Administration of sodium bicarbonate in the drinking water increased the measured tumor pH to 7.02 ± 0.04 (n = 5) (P < 0.01). Gavage with ammonium chloride decreased the pH to 6.47 ± 0.11 (n = 6) (P < 0.01). The pH_i_, estimated from the chemical shift of the intracellular inorganic phosphate resonance, was 7.44 ± 0.16 in untreated animals (n = 7) and was similar in mice treated with bicarbonate (7.47 ± 0.15 (n = 4) (P = 0.75)) or ammonium chloride (7.36 ± 0.08 (n = 6) (P = 0.30)). Correlation between the tumor pH determined with hyperpolarized H^13^CO_3_^-^ and the pH determined with the 3-APP probe suggested that hyperpolarized H^13^CO_3_^-^ predominantly measured the pH_e_. This probably reflects the higher concentration of extracellular versus intracellular bicarbonate, as well as the rapid acquisition of spectra immediately after injection of hyperpolarized bicarbonate. Bicarbonate injection did not significantly change the tumor pH_e_ as shown with 3-APP–based ^31^P MRS measurement (pH change = 0.02 ± 0.03; n = 4). Superimposition of the pH maps over the corresponding proton image of tissue water showed that the highest concentration of ^13^CO_2_ was in the tumor. The H^13^CO_3_^-^ signal was highest in the aorta, and there was little difference in signal intensities between muscle and tumor.

Signal from the hyperpolarized nuclear spin decreases rapidly because of the decay of polarization; thus it is possible that small differences in the rate at which H^13^CO_3_^-^ and ^13^CO_2_ lose polarization will lead to variations in the calculated pH with time. In the study by Gallagher et al., this was not observed over a period of 20 s measurement in vivo (data not shown) and could be explained by the fact that H^13^CO_3_^-^ and ^13^CO_2_ are interconverted so rapidly that their apparent T_1_ values become equal (4). The measured T_1_ was 10.1 ± 2.9 s (n = 9) for H^13^CO_3_^-^ and 9.8 ± 2.5 s for ^13^CO_2_ (n = 7) (P = 0.83). Theoretically, in the absence of ^13^CO_2_ resonance saturation, decay of the H^13^CO_3_^-^ resonance will be dominated by its T_1_. In the presence of ^13^CO_2_ resonance saturation, the H^13^CO_3_^-^ signal will decay with a time constant given by 1/(1/T_1_ + k), where k is the rate constant for the conversion of H^13^CO_3_^-^ to ^13^CO_2_. Gallagher et al. showed that inhibition of the carbonic anhydrase with acetazolamide abolished this decrease in the H^13^CO_3_^-^ signal, demonstrating the importance of the enzyme for the exchange of polarization between the two molecules (4). The apparent exchange rate constant was approximately eight times greater than the polarization loss rate constant (1/T_1_).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Gallagher F.A., Kettunen M.I., Hu D.E., Jensen P.R., Zandt R.I., Karlsson M., Gisselsson A., Nelson S.K., Witney T.H., Bohndiek S.E., Hansson G., Peitersen T., Lerche M.H., Brindle K.M. (2009). Production of hyperpolarized [1,4-13C2]malate from [1,4-13C2]fumarate is a marker of cell necrosis and treatment response in tumors. Proc Natl Acad Sci U S A.
2 Kurhanewicz J., Bok R., Nelson S.J., Vigneron D.B. (2008). Current and potential applications of clinical 13C MR spectroscopy. J Nucl Med.
3 Mansson S., Johansson E., Magnusson P., Chai C.M., Hansson G., Petersson J.S., Stahlberg F., Golman K. (2006). 13C imaging-a new diagnostic platform. Eur Radiol.
4 Gallagher F.A., Kettunen M.I., Day S.E., Hu D.E., Ardenkjaer-Larsen J.H., Zandt R., Jensen P.R., Karlsson M., Golman K., Lerche M.H., Brindle K.M. (2008). Magnetic resonance imaging of pH in vivo using hyperpolarized 13C-labelled bicarbonate. Nature.
5 Chen A.P., Tropp J., Hurd R.E., Van Criekinge M., Carvajal L.G., Xu D., Kurhanewicz J., Vigneron D.B. (2009). In vivo hyperpolarized 13C MR spectroscopic imaging with 1H decoupling. J Magn Reson.
6 Ardenkjaer-Larsen J.H., Fridlund B., Gram A., Hansson G., Hansson L., Lerche M.H., Servin R., Thaning M., Golman K. (2003). Increase in signal-to-noise ratio of > 10,000 times in liquid-state NMR. Proc Natl Acad Sci U S A.
7 Golman K., Ardenkjaer-Larsen J.H., Petersson J.S., Mansson S., Leunbach I. (2003). Molecular imaging with endogenous substances. Proc Natl Acad Sci U S A.
8 Larson P.E., Kerr A.B., Chen A.P., Lustig M.S., Zierhut M.L., Hu S., Cunningham C.H., Pauly J.M., Kurhanewicz J., Vigneron D.B. (2008). Multiband excitation pulses for hyperpolarized 13C dynamic chemical-shift imaging. J Magn Reson.
9 Golman K., Olsson L.E., Axelsson O., Mansson S., Karlsson M., Petersson J.S. (2003). Molecular imaging using hyperpolarized 13C. Br J Radiol.
10 Olsson L.E., Chai C.M., Axelsson O., Karlsson M., Golman K., Petersson J.S. (2006). MR coronary angiography in pigs with intraarterial injections of a hyperpolarized 13C substance. Magn Reson Med.
11 Albers M.J., Bok R., Chen A.P., Cunningham C.H., Zierhut M.L., Zhang V.Y., Kohler S.J., Tropp J., Hurd R.E., Yen Y.F., Nelson S.J., Vigneron D.B., Kurhanewicz J. (2008). Hyperpolarized 13C lactate, pyruvate, and alanine: noninvasive biomarkers for prostate cancer detection and grading. Cancer Res.
12 Chen A.P., Kurhanewicz J., Bok R., Xu D., Joun D., Zhang V., Nelson S.J., Hurd R.E., Vigneron D.B. (2008). Feasibility of using hyperpolarized [1-13C]lactate as a substrate for in vivo metabolic 13C MRSI studies. Magn Reson Imaging.
13 Karlsson, M., P.R. Jensen, R.I. Zandt, A. Gisselsson, G. Hansson, J.O. Duus, S. Meier, and M.H. Lerche, Imaging of branched chain amino acid metabolism in tumors with hyperpolarized (13)C ketoisocaproate. Int J Cancer, 2009
14 Jensen P.R., Karlsson M., Meier S., Duus J.O., Lerche M.H. (2009). Hyperpolarized amino acids for in vivo assays of transaminase activity. Chemistry.
15 Schroeder, M.A., P. Swietach, H.J. Atherton, F.A. Gallagher, P. Lee, G.K. Radda, K. Clarke, and D.J. Tyler, Measuring intracellular pH in the heart using hyperpolarized carbon dioxide and bicarbonate: a 13C and 31P magnetic resonance spectroscopy study. Cardiovasc Res.
16 Fukumura D., Jain R.K. (2007). Tumor microenvironment abnormalities: causes, consequences, and strategies to normalize. J Cell Biochem.
17 Izumi H., Torigoe T., Ishiguchi H., Uramoto H., Yoshida Y., Tanabe M., Ise T., Murakami T., Yoshida T., Nomoto M., Kohno K. (2003). Cellular pH regulators: potentially promising molecular targets for cancer chemotherapy. Cancer Treat Rev.
18 Gillies R.J., Liu Z., Bhujwalla Z. (1994). 31P-MRS measurements of extracellular pH of tumors using 3-aminopropylphosphonate. Am J Physiol.
19 van Sluis R., Bhujwalla Z.M., Raghunand N., Ballesteros P., Alvarez J., Cerdan S., Galons J.P., Gillies R.J. (1999). In vivo imaging of extracellular pH using 1H MRSI. Magn Reson Med.
20 Raghunand N., Zhang S., Sherry A.D., Gillies R.J. (2002). In vivo magnetic resonance imaging of tissue pH using a novel pH-sensitive contrast agent, GdDOTA-4AmP. Acad Radiol.
21 Vavere A.L., Biddlecombe G.B., Spees W.M., Garbow J.R., Wijesinghe D., Andreev O.A., Engelman D.M., Reshetnyak Y.K., Lewis J.S. (2009). A novel technology for the imaging of acidic prostate tumors by positron emission tomography. Cancer Res.
22 Tang J., Gai F. (2008). Dissecting the membrane binding and insertion kinetics of a pHLIP peptide. Biochemistry.
23 Andreev O.A., Dupuy A.D., Segala M., Sandugu S., Serra D.A., Chichester C.O., Engelman D.M., Reshetnyak Y.K. (2007). Mechanism and uses of a membrane peptide that targets tumors and other acidic tissues in vivo. Proc Natl Acad Sci U S A.